# Ethyl 8-fluoro-5-[^11^C]methyl-6-oxo-4H-imidazo[1,5-a][1,4]benzodiazepine-3-carboxylate

Chemical name: | Ethyl 8-fluoro-5-[^11^C]methyl-6-oxo-4H-imidazo[1,5-a][1,4]benzodiazepine-3-carboxylate
Abbreviated name: | [^11^C]FMZ
Synonym: | [^11^C]Flumazenil; Romazicon®; Ro 15-5528
Agent Category: | Compound
Target: | Gamma-aminobutyric acid type A receptors (GABA_A_ receptors)
Target Category: | Ligand-receptor binding
Method of detection: | Positron emission tomography (PET)
Source of Signal/Contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+Flumazenil)]

The development of epilepsy has been associated with the impairment of gamma-aminobutyric acid (GABA) neurotransmission in the central nervous system because a reduced GABA release has been observed in the mesial temporal lobe during epilepsy episodes in animals and a GABA-mediated inhibition loss was reported in human epileptic hippocampal sclerosis (1, 2). The GABA receptors (GABAR) comprise several different pharmacological subtypes depending on the type of subunits constituting the receptor complex, and GABA mediates its effects primarily through the GABA_A_ receptors (3). Also, individuals with the Angleman syndrome (AS) have a neurodevelopmental disorder that results in severe mental retardation, delayed motor development, and epilepsy (4). It has been shown that surviving gabrag3-knockout mice are epileptic and have a phenotype that is similar to AS patients, indicating that the GABRβ3 gene in humans could have a role in the development of AS (5). Interestingly, genes coding for the various GABAR subunits (β3, α5, and γ3) are located within the same 15q11-q13 region of the human chromosome that is believed to have a function in the development of AS (5, 6), suggesting that the GABARβ3 gene may have a role in the development of AS in humans. In addition, the GABA_A_knockout mice were shown to have reduced levels of the GABA_A_ receptor.

A benzodiazepine (BDZ) site antagonist labeled with radioactive carbon ([^11^C]), ethyl 8-fluoro-5-[^11^C]methyl-6-oxo-4H-imidazo[1,5-a][1,4]benzodiazepine-3-carboxylate ([^11^C]flumazenil ([^11^C]FMZ)), which has a high affinity for the GABA_A_ receptors, has been used widely with positron emission tomography (PET) for the investigation of the these receptors (7). Flumazenil is available commercially (http://www.rxlist.com/cgi/generic/flumazenil.htm) in the United States and has been approved by the United States Food and Drug Administration for use in various clinical trials (http://clinicaltrials.gov/ct2/results?term=flumazenil).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+flumazenil+synthesis)]

The synthesis of [^11^C]FMZ has been described by Nagren and Halldin (8). Briefly, 8-fluoro-5,6-dihydro-6-oxo-4H-imidazo[1,5-a][1,4]benzodiazepine-3-carboxylic acid (also known as desmethylflumazenil or desmethyl-FMZ or Ro 15-5528) was mixed with [^11^C]methyl triflate in a sealed reaction vessel at 0°C containing sodium hydroxide and acetone. The vessel was heated to 60°C for 1 min, and a mixture of acetonitrile:0.01 M phosphoric acid was injected into the vessel. The mixture was separated on a Waters reverse-phase high-performance liquid chromatography μ-Bondapak-C_18_ column, and the purified product was collected in a propylene glycol/ethanol mixture. The mobile phase was evaporated, and the residue was dissolved in propylene glycol/ethanol contained in physiological phosphate buffer (pH 7.4) and sterile filtered. The radiochemical yield (decay corrected) of this reaction was reported to be 65–75%. The radiochemical purity and specific activity of the product were not provided (8).

A robotic method for the synthesis of [^11^C]FMZ has also been published (9). The synthesis was performed on an Anatech RB 86 robotic system in a vial containing Ro 15-5528, potassium fluoride, and aluminum oxide in acetonitrile (9). [^11^C]Methyl iodide was trapped for 90 s in the vial, and the reaction mixture was kept at room temperature for another 120 s. A solid-phase extraction technique was used to separate [^11^C]FMZ from its precursor (Ro 15-5528). This was followed by removal of the solvent in a stream of nitrogen at 130°C. The purified [^11^C]FMZ was dissolved in an ethanol:saline mixture, and the solution was sterile filtered. The synthesis time was reported to be 30 min from the time of [^11^C]methyl iodide trapping. The radiochemical purity of [^11^C]FMZ was reported to be >99% with a specific activity of 11.1–59.2 GBq/μmol (0.3–1.6 Ci/μmol). The stability of the radiochemical was not reported (9).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11c+flumazenil+in+vitro)]

The in vitro characteristics of [^11^C]Ro 15-1788 were studied in membranes isolated from the rat forebrain (10). The various kinetic constants were determined with two different techniques involving a phosphorimager and γ-counter measurements. The dissociation constants (K_D_) were reported to be 2.0 ± 0.9 and 2.1 ± 0.5 nM, respectively, by the two methods, and the number of binding sites (B_max_) was determined to be 1.3 ± 0.5 and 1.7 ± 0.3 pmol/mg protein by the respective methods. In competition experiments the 50% inhibitory concentration (IC_50_) of unlabelled Ro 15-1788 was reported to be 4.03 ± 0.75 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+flumazenil+rodentia)]

Using [^11^C]FMZ, investigators have shown that the binding potential (B_max_/K_D_) of the GABA_A_ receptors is reduced significantly over a 12-h period in the trauma-site cortex of rats subjected to a moderate lateral fluid percussion injury (11). This demonstrated that the GABA receptors were involved in cellular dysfunction as a result of the fluid percussion injury in these animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+flumazenil+non-human+primates)]

Matsunaga et al. investigated the effect of yohimbine administration on BDZ receptor binding in the central nervous system of non-human primates (rhesus monkeys) (12). Using [^11^C]FMZ, the investigators reported that yohimbine, an α2-adrenoceptor antagonist, increased the binding potential for the BDZ receptors in the monkey brain, indicating that a state of anxiety potentiated the effects of anxiolytics.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=11C+flumazenil+humans)]

Using [^11^C]FMZ with PET in 11 patients with acute hemispheric ischemic stroke, Heiss et al. showed that this radiopharmaceutical is a suitable agent to distinguish between irreversibly damaged and viable neuronal tissue during early onset of the condition (13). In another study in 12 patients, the probability of predicting the cortical infarction in early ischemic stroke using PET versus diffusion-weighted magnetic resonance imaging (based on movement of water molecules, which is the method of choice to detect ischemic lesions) for the central BDZ receptors with [^11^C]FMZ was determined (14). With results obtained from this study, the investigators concluded that, although the two methods were comparable, the probability of false-positive predictions were lower when PET with [^11^C]FMZ was used.

Koepp et al. used [^11^C]FMZ to demonstrate a reduction in the number of GABA/central BDZ receptors in the hippocampus of patients with mesial temporal lobe epilepsy caused by unilateral hippocampal sclerosis (15). These observations were later confirmed by comparing in vivo [^11^C]FMZ and ex vivo [^3^H]FMZ binding in patients with hippocampal sclerosis with anterior temporal lobe resections (7).

[^11^C]FMZ has also been used to estimate the synaptic density of BZD in five individuals who became blind at an early age (16). Compared with sighted control subjects, a significantly lower (P < 0.01) BDZ density was reported in the cerebellum of the blind subjects. However, the BZD density was comparable in the visual areas and other cortical regions of the blind patients and the controls, indicating a modification of the cerebellar neural circuitry in the blind individuals.

The binding of [^11^C]FMZ was studied in four AS patients (17). Among these patients, three had a maternal deletion of 15q11-q13 leading to a loss of the β_3_ subunit of the GABAR, and the fourth patient had a mutation in the ubiquitin protein ligase (UBE3A) but had a normal β_3_ subunit gene. Compared to the fourth patient, a lower binding of [^11^C]FMZ was observed in the frontal, parietal, hippocampal, and cerebellar regions of the brain of the first three patients, indicating that the 15q11-q13 deletion leads to a reduced number of GABAR in the AS patients. However, using [^11^C]FMZ, Asahina et al. reported an increase in total expression of GABA_A_ receptors in the cerebral cortex and the cerebellum of five AS patients with a deletion and one patient with a UBE3A mutation (18).

## Supplemental Information

[Disclaimers]

## References

1 During M.J., Ryder K.M., Spencer D.D. (1995). Hippocampal GABA transporter function in temporal-lobe epilepsy. Nature.
2 Knowles W.D., Awad I.A., Nayel M.H. (1992). Differences of in vitro electrophysiology of hippocampal neurons from epileptic patients with mesiotemporal sclerosis versus structural lesions. Epilepsia.
3 Luddens H., Korpi E.R., Seeburg P.H. (1995). GABAA/benzodiazepine receptor heterogeneity: neurophysiological implications. Neuropharmacology.
4 Moncla A., Malzac P., Voelckel M.A., Auquier P., Girardot L., Mattei M.G., Philip N., Mattei J.F., Lalande M., Livet M.O. (1999). Phenotype-genotype correlation in 20 deletion and 20 non-deletion Angelman syndrome patients. Eur J Hum Genet.
5 DeLorey T.M., Handforth A., Anagnostaras S.G., Homanics G.E., Minassian B.A., Asatourian A., Fanselow M.S., Delgado-Escueta A., Ellison G.D., Olsen R.W. (1998). Mice lacking the beta3 subunit of the GABAA receptor have the epilepsy phenotype and many of the behavioral characteristics of Angelman syndrome. J Neurosci.
6 Glatt K., Glatt H., Lalande M. (1997). Structure and organization of GABRB3 and GABRA5. Genomics.
7 Koepp M.J., Hand K.S., Labbe C., Richardson M.P., Van Paesschen W., Baird V.H., Cunningham V.J., Bowery N.G., Brooks D.J., Duncan J.S. (1998). In vivo [11C]flumazenil-PET correlates with ex vivo [3H]flumazenil autoradiography in hippocampal sclerosis. Ann Neurol.
8 Nagren K., Halldin C. (1998). Methylation of amide and thiol functions with [11C]methyltriflate, as examplified by [11C]NMSP, [11C]flumazenil and [11C]methionine. Journal of Labelled Compounds and radiopharmaceuticals.
9 Krasikova R., Fedorova O., Korsakov M., Nagren K., Maziere B., Halldin C. (2000). A fast and convenient method for robotic preparation of [11C]flumazenil avoiding HPLC purification. Journal of Labelled Compounds and Radiopharmaceuticals.
10 Sihver W., Sihver S., Bergstrom M., Murata T., Matsumura K., Onoe H., Andersson Y., Bjurling P., Fasth K.J., Westerberg G., Ogren M., Jacobsson G., Lundqvist H., Oreland L., Watanabe Y., Langstrom B. (1997). Methodological aspects for in vitro characterization of receptor binding using 11C-labeled receptor ligands: a detailed study with the benzodiazepine receptor antagonist [11C]Ro 15-1788. Nucl Med Biol.
11 Sihver S., Marklund N., Hillered L., Langstrom B., Watanabe Y., Bergstrom M. (2001). Changes in mACh, NMDA and GABA(A) receptor binding after lateral fluid-percussion injury: in vitro autoradiography of rat brain frozen sections. J Neurochem.
12 Matsunaga T., Tsukada H., Nishiyama S., Sekine Y., Kakiuchi T., Iyo M., Mori N. (2001). Yohimbine increases the binding potential for [11C]flumazenil in the monkey brain. J Neural Transm.
13 Heiss W.D., Kracht L., Grond M., Rudolf J., Bauer B., Wienhard K., Pawlik G. (2000). Early [(11)C]Flumazenil/H(2)O positron emission tomography predicts irreversible ischemic cortical damage in stroke patients receiving acute thrombolytic therapy. Stroke.
14 Heiss W.D., Sobesky J., Smekal U., Kracht L.W., Lehnhardt F.G., Thiel A., Jacobs A.H., Lackner K. (2004). Probability of cortical infarction predicted by flumazenil binding and diffusion-weighted imaging signal intensity: a comparative positron emission tomography/magnetic resonance imaging study in early ischemic stroke. Stroke.
15 Koepp M.J., Richardson M.P., Brooks D.J., Poline J.B., Van Paesschen W., Friston K.J., Duncan J.S. (1996). Cerebral benzodiazepine receptors in hippocampal sclerosis. An objective in vivo analysis. Brain.
16 Sanabria-Bohorquez S.M., De Volder A.G., Arno P., Sibomana M., Coppens A., Michel C., Veraart C. (2001). Decreased benzodiazepine receptor density in the cerebellum of early blind human subjects. Brain Res.
17 Holopainen I.E., Metsahonkala E.L., Kokkonen H., Parkkola R.K., Manner T.E., Nagren K., Korpi E.R. (2001). Decreased binding of [11C]flumazenil in Angelman syndrome patients with GABA(A) receptor beta3 subunit deletions. Ann Neurol.
18. Asahina, N., T. Shiga, K. Egawa, H. Shiraishi, S. Kohsaka, and S. Saitoh, [(11)C]flumazenil positron emission tomography analyses of brain gamma-aminobutyric acid type A receptors in Angelman syndrome. J Pediatr, 2008. 152(4): p. 546-9, 549 e1-3.